# Gadolinium-labeled diethylenetriamine pentaacetic acid-CGLIIQKNEC

Chemical name: | Gadolinium-labeled diethylenetriamine pentaacetic acid-CGLIIQKNEC
Abbreviated name: | Gd-DTPA-CLT1
Synonym:
Agent category: | Peptide
Target: | Fribrin-fibronectin clot complexes
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (2). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (3). A meshwork of clotted plasma protein was present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (4). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (5, 6). Gd-labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, they are largely nonspecific. CGLIIQKNEC (CLT1), a fibronectin-fibrin binding peptide, was identified with phage display screening (4). The peptide was conjugated with Gd-DTPA to form Gd-DTPA-CLT1 for imaging of fibronectin-fibrin complexes in tumor tissues (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+synthesis)]

DTPA-CLT1 was synthesized with solid-phase synthesis (7). DTPA was conjugated to the N-terminal of CLT1 peptide. Gd(OAc)_3_ and DTPA-CLT1 were incubated at pH 6. The product, Gd-DTPA-CLT1 (1:1:1), was isolated with high-performance liquid chromatography. The mass (m/z, M + H^+^) of Gd-DTPA-CLT1 was 1,650.75 as determined with mass spectrometry (calculated: 1,650.20).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+in+vitro)]

Gd-DTPA-CLT1 exhibited T1 and T2 relaxivity values of 4.22 mM^-1^ and 4.45 mM^-1^ at 3T, respectively (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+rodentia)]

Ye et al. (7) performed dynamic T1-weighted MRI studies with 100 nmol/kg Gd-DTPA-CLT1 in mice (n = 3) bearing HT-29 xenografts. Gd-DTPA-bismethylamide (100 nmol/kg) was used a control contrast agent. Contrast-enhanced MRI images were obtained before injection and at 1, 10, 30, and 60 min after injection. Enhanced contrast in the tumor tissues was visualized for Gd-DTPA-CLT1 at 10–60 min after injection. Pretreatment with CLT1 (300 nmol/kg) reduced the Gd-DTPA-CLT1 enhancement. Gd-DTPA-bismethylamide exhibited weaker enhancement in the tumor tissues as compared with Gd-DTPA-CLT1. The contrast/noise ratio (CNR) at the tumor periphery was higher than in the tumor inner area at 10 min after injection of Gd-DTPA-CLT1 and decreased gradually. At the same time, the CNR in the tumor inner area increased over the next 50 min. On the other hand, Gd-DTPA-bismethylamide exhibited the maximal CNR at 1 min after injection at the tumor periphery and in the inner area and decreased rapidly thereafter. Gd-DTPA-CLT1 exhibited higher CNR than Gd-DTPA-BMA at the tumor periphery after 10 min (P < 0.05) and in the tumor inner area after 30 min (P < 0.05). Excess CLT1 reduced the CNR both at the tumor periphery and in the inner area. Histochemical staining localized fibronectin in the extracellular spaces in the tumor tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+human)]

No publication is currently available.

## NIH Support

R01 CA097465

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
3 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
4 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
5 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
6 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
7 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.